# Gly-Ser-Ser-Lys-(FITC)-Gly-Gly-Gly-Cys-Arg-Gly-Asp-Cys-CLIO-Cy5.5

Chemical name: | Gly-Ser-Ser-Lys-(FITC)-Gly-Gly-Gly-Cys-Arg-Gly-Asp-Cys-CLIO-Cy5.5
Abbreviated name: | cRGD-CLIO(Cy5.5)
Synonym:
Agent category: | Peptide, small molecule (nanoparticle)
Target: | α_υ_β_3_ integrin
Target category: | Receptor
Method of detection: | Magnetic resonance imaging (MRI), fluorescence molecular tomography (FMT), fluorescence reflectance imaging (FRI)
Source of signal/contrast: | Iron oxides, Cy5.5
Activation: | No
Studies: | - In vitro; - Rodents | No structure is available in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(cRGD-CLIO))]

The α_υ_β_3_ integrin, also known as the vitronectin receptor, is a heterodimeric transmembrane glycoprotein found on most cells originating from mesenchyme (1). This receptor is often overexpressed in various tumor cells, including osteosarcomas, neuroblastomas, glioblastomas, invasive melanomas, and carcinomas of the lung, breast, prostate, and bladder (1). Many extracellular matrix proteins such as fibronectin, vitronectin, thrombospondin, fibrinogen, osteopontin, and tenascin are known to be involved in interactions with various subtypes of integrins (1). These proteins may contain a variety of motifs for potential cell binding; however, one of the most frequent cell-recognition motifs includes an amino acid sequence of Arg-Gly-Asp (RGD), called “the universal cell-recognition site” (1) or “a versatile cell recognition signal” (2). The binding potency of the RGD motif leads to the development of small homing peptides, whose high affinity to the α_υ_β_3_ integrin provides a promising alternative to antibodies in targeting tumors (3). As a result, RGD analogs are widely used in tumor imaging, anti-angiogenesis treatment, and tumor-associated radionucleotides or chemotherapeutic drugs. Some RGD analogs are currently being used in phase II clinical trials (4). These α_υ_β_3_ integrin–specific probes will help oncologists improve the delineation of tumors and follow up the progression of anti-angiogenic therapies (4).

Gly-Ser-Ser-Lys-(FITC)-Gly-Gly-Gly-Cys-Arg-Gly-Asp-Cys-cross-linked iron oxide-Cy5.5 (cRGD-CLIO(Cy5.5)) is a magneto-fluorescent nanoparticle for multimodal imaging of α_υ_β_3_ integrin. This agent consists of three components: an RGD peptide for targeting α_υ_β_3_ integrin, two fluorescence probes for optical detection/imaging, and an iron oxide nanoparticle core for magnetic resonance imaging (MRI) contrast enhancement (5). The peptide contains 12 amino acids with an intramolecular disulfide bond to form a cyclic RGD (cRGD). One of the fluorescence probes, fluorescein isothiocyanate (FITC), is attached to the peptide before conjugation to the nanoparticle, allowing for the characterization of peptide/iron ratio and the quantification of cell-associated peptide or peptide-nanoparticle on the basis of the absorption at 493 nm. The other fluorescence probes (i.e., Cy5.5 or Cy3.5) are cyanine dyes consisting of two quaternized heteroaromatic bases (A and A’) joined by a polymethine chain with five (Cy5.5) or three (Cy3.5) carbons (6) and directly bound to the nanoparticle (5). These dyes have a cationic character because of the delocalized positive charge of the chromophore, and they possess high quantum yield, good chemical stability, easy conjugation, and high sensitivity (mole extinction coefficient ~ 250,000 mol/cm) (7, 8). The excitation/emission wavelength is 674/692 nm for Cy5.5 and 548/563 nm for Cy3.5, where hemoglobin and water have their lowest absorption coefficient. The difference in wavelength of Cy5.5/Cy3.5 allows for dual wavelength ratio imaging to quantify the components labeled with Cy5.5 or Cy3.5 (9).

The nanoparticle contains an icosahedral core of superparamagnetic crystalline Fe_3_O_4_ (magnetite) (10) that is caged by epichlorohydrin cross-linked dextran and functionalized with amine groups (CLIO-NH_2_) (11). These amino groups are used in further conjugation chemistry for attaching the RGD peptides and the fluorescent dyes. The superparamagnetic crystalline includes a sufficiently large single-domain of unpaired spins to generate a net magnetic moment that is larger than the sum of its individual unpaired electrons (10, 12). The main difference between these superparamagnetic nanoparticles and paramagnetic ions such as gadolinium (Gd) is their large magnetic moment unhindered by lattice orientation (13). Thus, they possess a high magnetic susceptibility that results in a significant induced magnetization inside a magnetic field. This, in turn, creates microscopic field gradients that diphase nearby protons and cause T_2_ shortening (13). CLIO-NH_2_ has a magnetite core of ~5 nm with a hydrodynamic diameter of 20 nm (11, 12), which can lead to a three- to four-fold increase in T_1_ relaxivity and a five- to six-fold increase in T_2_ relaxivity compared to conventional contrast agents such as Gd-diethylenetriamine pentaacetic acid (Gd-DTPA) (10). CLIO-NH_2_ is suitable for receptor-directed MRI or magnetically labeled cell probe MRI because it is small enough to easily pass through capillary endothelium while retaining superparamagnetism (12). Despite its small size, CLIO still exhibits superparamagnetic properties and is detectable at tissue concentrations of only 50 nmol Fe/g tissue (10^13–14^ iron particles/g tissue) (10).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(cRGD-CLIO)+AND+synthesis%0D%0A)]

Montet et al. reported a detailed synthesis of cRGD-CLIO(Cy5.5) (5). Initially, a linear RGD peptide GSSK(FI)GGGCRGDC (IRGD) was obtained with the Fmoc method as a C-terminal amide and oxidized via bubbling air to yield a disulfide-linked cRGD peptide in 0.1 M ammonium bicarbonate. The amino-CLIO nanoparticle was synthesized in several steps. The starting material, monocrystalline iron oxide (MION), was synthesized by neutralization of ferrous salts, ferric salts, and dextran with ammonium hydroxide, followed by ultra-filtration (14). The obtained MION was cross-linked in strong base with epichlorohydrin and then reacted with ammonia to produce amino-CLIO (CLIO-NH_2_) (14). Finally, CLIO-NH_2_ was reacted with the N-hydroxysuccinimide ester of Cy5.5 (Amersham Biosciences Corp., Piscataway, NJ), followed by peptide attachment using disuccinimidyl suberimidate to produce cRGD-CLIO(Cy5.5) (5). There were ~250 amines, 8,000 iron atoms, 27 peptides, and 8 Cy5.5 molecules per CLIO-NH_2_ nanoparticle.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(cRGD-CLIO)+AND+%22in+vitro%22)]

The uptake of cRGD-CLIO(Cy5.5) was examined in human breast carcinomas (BT-20) by iron stain or Cy5.5 fluorescence (5). After injection of nanoparticles, iron and fluorescence were broadly distributed through the tumor. The molecular specificity for cRGD-CLIO(Cy5.5) binding to α_υ_β_3_ integrin was determined in BT-20 cells (5). First, the 50% effective concentration (EC_50_) of cRGD-CLIO(Cy5.5) was compared with that of IRGD-CLIO(Cy5.5) when they were bound to the BT-20 cells. The EC_50_ was found to be 0.0113 μM for the cyclic isomer and 0.4 μM for the linear isomer using a fluorescence-activated cell-sorting (FACS) cytometer. This demonstrated that the cRGD had a 35-fold increase in affinity compared to the linear RGD. Second, the binding affinity of cRGD-CLIO(Cy5.5) was compared with that of a scrambled peptide analog (srcRGD-CLIO(Cy3.5)) by measuring their uptake in the BT-20 tumor. Animals with tumors were euthanized 24 h after intravenous injection of mixed cRGD-CLIO(Cy5.5) and srcRGD-CLIO(Cy3.5) at 5 mg Fe/kg dose, and slices of tissues were imaged with a multichannel fluorescent imager. The Cy5.5/Cy3.5 ratio was found to be 6.5 in the BT-20 tumor and ~1 in the liver or spleen, where a high concentration of nanoparticles accumulated. The distribution of cRGD-CLIO(Cy5.5) in the BT-20 tumor was illustrated with iron staining and fluorescence microscopy, in which both iron and Cy5.5 fluorescence were observed throughout the whole tumor.

The expression of α_υ_β_3_ integrin in rat gliosarcomas (9L) was first examined with cRGD alone by fluorescein immunoassay (5). The apparent affinity constant of cRGD-CLIO in the 9L cells was very similar to that in the BT-20 cells, but the maximum amount (B_max_) of cRGD bound to α_υ_β_3_ integrin was 0.16 pmol in the 9L cells, which is about four times lower than the 0.82 pmol in the BT-20 cells. This indicated that expression of the α_υ_β_3_ integrin in the 9L tumor was four times less than that in the BT-20 tumors. Then, the binding affinity of cRGD-CLIO(Cy5.5) in the 9L tumors was compared with that of srcRGD-CLIO(Cy3.5). The Cy5.5/Cy3.5 fluorescence ratio was 1.8, which was 3.6 times lower than that in the BT-20 tumor. In addition, the cRGD-CLIO(Cy5.5) was found to have a hydrodynamic diameter of 28 ± 3 nm with a T_2_ relaxivity of 111 mM^-1^s^-1^ at 4.7 T (5).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(cRGD-CLIO) +AND++rodentia)]

cRGD-CLIO (Cy5.5) was used to examine the expression of α_υ_β_3_ integrin in BT-20 tumors (3–4 mm in diameter) implanted in nude mice. Fluorescence reflectance imaging (FRI) was conducted after intravenous injection of cRGD-CLIO(Cy5.5)/srcRGD-CLIO(Cy3.5) at 5 mg Fe/kg. FRI showed a much higher tumor/background ratio at the Cy5.5 channel than at the Cy3.5 channel during the first 1,500 min after injection. Because the blood half-life time of cRGD-CLIO(Cy5.5) was 180 mins, the signal enhancement in the Cy5.5 channel reflected the accumulation of cRGD-CLIO(Cy5.5) in the tumor cells. Fluorescence molecular tomography (FMT) and MRI at 4.7 T were performed after intravenous injection of 3 mg Fe/kg cRGD-CLIO(Cy5.5). FMT images demonstrated different enhancements for deep tumor slices. MRI images exhibited an apparent T_2_-shortening effect caused by cRGD-CLIO(Cy5.5) because the mean tumor T_2_ dropped from 77 ms before injection to 66 ms 24 h after injection.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22%20SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(cRGD-CLIO) +AND+(primate+non+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(cRGD-CLIO) +AND+human)]

No publication is currently available.

### NIH Support

P50 CA86355, R24 CA92782, R01 EB00662

## References

1 Haubner R., Finsinger D., Kessler H. (1997). Stereoisomeric peptide libaries and peptidomimetics for designing selective inhibitors of the aub3 integrin for a new cancer therapy. Angew. Chem. Int. Ed. Engl.
2 Ruoslahti E., Pierschbacher M.D. (1986). Arg-Gly-Asp: a versatile cell recognition signal. Cell.
3 Zitzmann S., Ehemann V., Schwab M. (2002). Arginine-glycine-aspartic acid (RGD)-peptide binds to both tumor and tumor-endothelial cells in vivo. Cancer Res.
4 Garanger E., Boturyn D., Dumy P. (2007). Tumor targeting with RGD peptide ligands-design of new molecular conjugates for imaging and therapy of cancers. Anticancer Agents Med Chem.
5 Montet X., Montet-Abou K., Reynolds F., Weissleder R., Josephson L. (2006). Nanoparticle imaging of integrins on tumor cells. Neoplasia.
6 Ernst L.A., Gupta R.K., Mujumdar R.B., Waggoner A.S. (1989). Cyanine dye labeling reagents for sulfhydryl groups. Cytometry.
7 Lin Y., Weissleder R., Tung C.H. (2002). Novel near-infrared cyanine fluorochromes: synthesis, properties, and bioconjugation. Bioconjug Chem.
8 Ballou B., Fisher G.W., Hakala T.R., Farkas D.L. (1997). Tumor detection and visualization using cyanine fluorochrome-labeled antibodies. Biotechnol Prog.
9 Kircher M.F., Josephson L., Weissleder R. (2002). Ratio imaging of enzyme activity using dual wavelength optical reporters. Mol Imaging.
10 Shen T., Weissleder R., Papisov M., Bogdanov A., Brady T.J. (1993). Monocrystalline iron oxide nanocompounds (MION): physicochemical properties. Magn Reson Med.
11 Josephson L., Perez J.M., Weissleder R. (2001). Magnetic nanosensors for the detection of oligonucleotide sequences. Angew. Chem. Int. Ed. Engl.
12 Wang Y.X., Hussain S.M., Krestin G.P. (2001). Superparamagnetic iron oxide contrast agents: physicochemical characteristics and applications in MR imaging. Eur Radiol.
13 Bulte J.W. Brooks R.A. Moskowitz B.M. Bryant L.H. Jr Frank J.A. T1 and T2 relaxometry of monocrystalline iron oxide nanoparticles (MION-46L): theory and experiment Acad Radiol 1998 5Suppl 1S137 40 9561064
14 Wunderbaldinger P. Josephson L. Weissleder R. Crosslinked iron oxides (CLIO): a new platform for the development of targeted MR contrast agents Acad Radiol 2002 9Suppl 2S304 6 12188255